# ^131^I-Human recombinant anti-ED-B fibronectin antibody small immunoprotein

Chemical name: | ^131^I-Human recombinant anti-ED-B fibronectin antibody small immunoprotein
Abbreviated name: | ^131^I-L19-SIP, ^131^I-SIP-L19
Synonym:
Agent category: | Single-chain Antibody fragment (ScFv)_2_
Target: | ED-B Fibronectin (FN)
Target category: | Adhesion molecule
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about ED-B fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L19-SIP)]

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels. Tumor growth depends on the formation of new blood vessels via this process. Tumor angiogenesis is important in the carcinogenesis, growth and progression of human solid tumors. Fibronectin (FN) are a widely distributed family of universal cell-adhesion molecules (1). FN is a polymorphic glycoprotein of ~2500 amino acids and has a high molecular mass of 250−280 kDa. FN occurs in soluble form in plasma and other body fluids and in insoluble form in the extracellular matrixes (2, 3). The splice variant ED-B FN is highly expressed during angiogenesis in vasculatures of tumor, normal and fetal tissues (4). In contrast, normal adult tissues do not express ED-B FN. High levels of ED-B FN expression have been found in vasculatures of breast, colorectal, and non-small cell lung tumors (1, 5-7).

Angiogenesis is essential for the growth of solid tumors and their metastases. Imaging angiogenesis may be useful for monitoring angiogenic treatments of tumors and cardiovascular diseases (8-10). A molecular probe that targets ED-B FN can be both an early tumor marker and a tool to monitor the success of antiangiogenic cancer therapy. The single-chain antibody fragment scFv L19, with a high affinity (K_d_ = 54 pM) to ED-B FN was developed by Pini et al. (11). Radioiodinated L19 showed specific accumulation around tumor neovasculature and tumor stroma with high ED-B expression (12, 13). Recently, a bispecific L19 was constructed by fusion of two L19 scFv fragments to form a divalent scFv small immunoprotein (L19-SIP, 80 kDa). Radiolabeled L19-SIP is being evaluated for imaging of neovasculature and radio-immunotherapy of cancer (14).

### Related Resource Links:

- Chapters in MICAD (Fibronectin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Fibronectin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), L19-SIP (http://www.ncbi.nlm.nih.gov/books/?term=L19-sip+AND+micad%5Bbook%5D))
- Gene information in NCBI (Fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Fibronectin (http://omim.org/entry/135600))
- Clinical trials (^131^I-L19-SIP (http://www.clinicaltrials.gov/ct2/results?term=L19-SIP))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I%20L19-SIP%20and%20synthesis)]

Borsi et al. (13) constructed L19-SIP divalent scFv fusion protein encoding an IgE C_H_4 domain for dimerization. Tijink et al. (14) performed iodination of L19-SIP with either ^125^I or ^131^I using the procedure as previously reported by Visser et al. (15). To a 20-mL vial coated with 75 µg IODO-GEN (1,3,4,6-tetrachloro-3α,6α-diphenyl-glycouril), 50 µL Na_2_HPO_4_ (0.5 M), 72–150 µg L19-SIP in 450 µL Na_2_HPO_4_ (0.1 M), and 6.7–11.1 MBq (0.18–0.3 mCi) ^125^I or ^131^I were added successively for a reaction of 4 min. Radiochemical yields were >70% after purification with PD-10 column chromatography. Specific activities were 56-62 MBq/mg (1.5–1.7 mCi/mg) with a radiochemical purity of >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I%20L19-SIP%20and%20in%20vitro)]

Tijink et al. (14) determined the in vitro immunoreactivity of ^125/131^I-L19-SIP by using affinity chromatography with ED-B FN-conjugated Sepharose column. The immunoreactivity of ^125/131^I-L19-SIP was always >70% at the highest ED-B–resin concentration and >95% at infinite antigen excess.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L19-SIP%20and%20rodentia)]

Tijink et al. (14) performed biodistribution studies of ^131^I-L19-SIP in nude mice bearing the human squamous cell carcinoma of the head and neck (HNSCC) FaDu (high ED-B expression) or HNX-OE (medium ED-B expression). Uptake of ^131^I-L19-SIP in FaDu tumors was higher than that in HNX-OE tumors. FaDu uptake values were 8.6 ± 1.6%ID/g at 24 h, 5.8 ± 0.4%ID/g, at 48 h, and 3.4 ± 0.2%ID/g at 74 h after injection. On the other hand, HNX-OE uptake values were 4.9 ± 1.1, 3.7 ± 0.7, and 2.5 ± 0.5%ID/g, respectively. ^131^I-L19-SIP showed rapid blood clearance and radioactivity localization in the tumor. The tumor/blood ratios were 4.4 ± 1.8 at 24 h and 21.4 ± 1.7 at 72 h for the FaDu xenografts, for the HNX-OE xenografts these ratios were 3.1 ± 1.2 at 24 h and 15.1 ± 1.5 at 72 h. Both the tumors exhibited the highest accumulation, followed by the urinary bladder and stomach.

Wyss et al. (16) determined uptake of ^131^I-L19-SIP, [^18^F]fluorocholine, [^18^F]fluoro-ethyl-l-tyrosine ([^18^F]FET), and 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG) in orthotopically induced C6 gliomas in 17 rats. The mean ^131^I-L19-SIP, [18F]fluorocholine, [^18^F]FET, and [^18^F]FDG standardized uptake values in the tumor and the contralateral normal cortex (in parentheses) were 0.31 ± 0.22 (not detectable), 2.00 ± 0.53 (0.49 ± 0.07), 3.67 ± 0.36 (1.42 ± 0.22), and 7.23 ± 1.22 (3.64 ± 0.51), respectively. The ^131^I-L19-SIP uptake pattern correlated best with [^18^F]fluorocholine uptake (z = 0.80, averaged z-transformed Pearson correlation coefficient) and [^18^F]FET uptake (z = 0.79) and least with [^18^F]FDG (z = 0.37).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L19-SIP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L19-SIP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L19-SIP%20and%20human)]

No publication is currently available.

## References

1 Berndorff D., Borkowski S., Moosmayer D., Viti F., Muller-Tiemann B., Sieger S., Friebe M., Hilger C.S., Zardi L., Neri D., Dinkelborg L.M. (2006). Imaging of tumor angiogenesis using 99mTc-labeled human recombinant anti-ED-B fibronectin antibody fragments. J Nucl Med.
2 Carnemolla B., Balza E., Siri A., Zardi L., Nicotra M.R., Bigotti A., Natali P.G. (1989). A tumor-associated fibronectin isoform generated by alternative splicing of messenger RNA precursors. J Cell Biol.
3 Kosmehl H., Berndt A., Katenkamp D. (1996). Molecular variants of fibronectin and laminin: structure, physiological occurrence and histopathological aspects. Virchows Arch.
4 Castellani P., Viale G., Dorcaratto A., Nicolo G., Kaczmarek J., Querze G., Zardi L. (1994). The fibronectin isoform containing the ED-B oncofetal domain: a marker of angiogenesis. Int J Cancer.
5 Kaczmarek J., Castellani P., Nicolo G., Spina B., Allemanni G., Zardi L. (1994). Distribution of oncofetal fibronectin isoforms in normal, hyperplastic and neoplastic human breast tissues. Int J Cancer.
6 Pujuguet P., Hammann A., Moutet M., Samuel J.L., Martin F., Martin M. (1996). Expression of fibronectin ED-A+ and ED-B+ isoforms by human and experimental colorectal cancer. Contribution of cancer cells and tumor-associated myofibroblasts. Am J Pathol.
7 Santimaria M., Moscatelli G., Viale G.L., Giovannoni L., Neri G., Viti F., Leprini A., Borsi L., Castellani P., Zardi L., Neri D., Riva P. (2003). Immunoscintigraphic detection of the ED-B domain of fibronectin, a marker of angiogenesis, in patients with cancer. Clin Cancer Res.
8 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
9 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
10 Miller J.C., Pien H.H., Sahani D., Sorensen A.G., Thrall J.H. (2005). Imaging angiogenesis: applications and potential for drug development. J Natl Cancer Inst.
11 Pini A., Viti F., Santucci A., Carnemolla B., Zardi L., Neri P., Neri D. (1998). Design and use of a phage display library. Human antibodies with subnanomolar affinity against a marker of angiogenesis eluted from a two-dimensional gel. J Biol Chem.
12 Tarli L., Balza E., Viti F., Borsi L., Castellani P., Berndorff D., Dinkelborg L., Neri D., Zardi L. (1999). A high-affinity human antibody that targets tumoral blood vessels. Blood.
13 Borsi L., Balza E., Bestagno M., Castellani P., Carnemolla B., Biro A., Leprini A., Sepulveda J., Burrone O., Neri D., Zardi L. (2002). Selective targeting of tumoral vasculature: comparison of different formats of an antibody (L19) to the ED-B domain of fibronectin. Int J Cancer.
14 Tijink B.M., Neri D., Leemans C.R., Budde M., Dinkelborg L.M., Stigter-van Walsum M., Zardi L., van Dongen G.A. (2006). Radioimmunotherapy of head and neck cancer xenografts using 131I-labeled antibody L19-SIP for selective targeting of tumor vasculature. J Nucl Med.
15 Visser G.W., Klok R.P., Gebbinck J.W., ter Linden T., van Dongen G.A., Molthoff C.F. (2001). Optimal quality (131)I-monoclonal antibodies on high-dose labeling in a large reaction volume and temporarily coating the antibody with IODO-GEN. J Nucl Med.
16 Wyss M.T., Spaeth N., Biollaz G., Pahnke J., Alessi P., Trachsel E., Treyer V., Weber B., Neri D., Buck A. (2007). Uptake of 18F-Fluorocholine, 18F-FET, and 18F-FDG in C6 Gliomas and Correlation with 131I-SIP(L19), a Marker of Angiogenesis. J Nucl Med.